# [^111^In]-Labeled chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX

Chemical name: | [^111^In]-Labeled chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX
Abbreviated name: | [^111^In]-DOTA-cG250
Synonym: | [^111^In]-DO3A-cG250; [^111^In]-cG250
Agent Category: | Antibody
Target: | Carbonic anhydrase IX
Target Category: | Enzyme
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[[underlined: PubMed]]

A common feature of most solid cancerous tumor types is the presence of hypoxic conditions (1) and the overexpression of carbonic anhydrase IX (CA IX), a transmembrane cell-surface enzyme that is known to regulate the pH and adhesion of tumor cells (2). Hypoxic tumors are often resistant to radio- and chemotherapy, have a high metastatic potential, and usually predict a poor outcome for the cancer patient (3). Although several methods (invasive and noninvasive) are available for the detection of hypoxia in tumors, including the use of radiolabeled small molecules, these methods are not completely reliable because they either yield variable diagnoses or have functional limitations due to incomplete penetration of tumors and fail to detect hypoxia in all tumor types (3, 4). Because CA IX is overexpressed in most solid tumors, it is considered to be a hypoxia biomarker, and targeting the CA IX for the detection of hypoxic tumors is of great interest to investigators (1, 3-5). A ^131^I-labeled murine monoclonal antibody (mAb) that targets the CA IX, designated G250, was developed and evaluated for the radiotherapy of metastatic renal cell carcinoma (RCC) patients, but no major responses were observed because the individuals developed immunity to the mAb (6). Subsequently, a ^131^I-labeled chimeric form of G250, [^131^I]-cG250, was developed and evaluated as an immunotherapeutic agent for the treatment of RCC (7). cG250 has been labeled with other nuclides (such as ^89^Zr, ^177^Lu, ^90^Y, etc.) and has been used in preclinical studies in rats (8) and for the treatment of RCC (7). However, only minor responses were observed in the clinical investigations, and dose escalation studies are ongoing (7).

Radiolabeled antibodies (Abs) have a limited ability to detect or treat cancer because these agents show only a peripheral penetration of solid tumors (due to a large size, ~150 kDa) and leave many neoplastic cells in the lesion untreated (9). In addition, Abs have prolonged blood circulation and present a high radiation dose risk to the bone marrow (10). In comparison, the smaller monovalent Fab (~50 kDa) and the divalent F(ab’)_2_ (~100 kDa) fragments derived from the parent Ab exhibit better tumor penetration and a shorter circulating half-life and are likely to yield better results if used to detect or treat solid malignant tumors (9). Between the two fragment types, the divalent F(ab’)_2_ fragments may more useful for the detection or treatment of malignant tumors because they have a higher affinity for the antigen (11). With these observations in mind, a divalent F(ab’)_2_ fragment of cG250 was developed, labeled with ^131^I, and compared with the intact [^131^I]-cG250 Ab for its pharmacokinetic behavior and its ability to target tumors in mice and RCC patients (10). However, from this study the investigators concluded that the intact Ab was superior to the divalent fragment for targeting the RCC tumors. A clinical trial to investigate the safety of a ^124^I-labeled version of cG250 in patients with renal masses has been reported (12). In addition cG250 is also under evaluation in several other clinical trials (http://clinicaltrials.gov/ct2/results?term=cG250). Recently, ^89^Zr-labeled F(ab’)_2_ fragments of cG250 were shown to be suitable for the visualization of hypoxic head and neck cancer xenograft tumors in mice (5).

Brouwers et al. compared the use of [^111^In]-isothiocynate-diethylenetriamine pentaacetic acid-cG250 and [^131^I]-cG250 for the detection of RCC metastases in five patients and concluded that the former tracer was superior to the latter for visualization of the tumors (13). In another study involving three patients, it was shown that neither ^131^I-labeled cG250 nor ^111^In-labeled cG250 were suitable for the radioimmunotherapy of biliary cancer (14). In a recent study using 1,4,7,10-tetraazacyclododecane-N,N’,N'',N’’’-tetraacetic acid (DOTA) as a nuclide conjugating agent, ^111^In-labeled cG250 Ab ([^111^In]-DOTA-cG250) and its Fab ([^111^In]-DOTA-Fab-cG250) and F(ab’)_2_ ([^111^In]-DOTA-F(ab’)_2_-cG250) fragments were generated and compared for their biodistribution and detection of hypoxic HT-29 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) (of human colorectal adenocarcinoma origin) xenograft tumors in mice (1).

This chapter details the studies performed with [^111^In]-DOTA-cG250. Studies performed with [^111^In]-DOTA-Fab-cG250 (15) and [^111^In]-DOTA-F(ab’)_2_-cG250 (16) are discussed in separate chapters of MICAD (www.micad.nih.gov).

### Other Sources of Information

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Carbonic+anhydrase+IX+inhibitors) on carbonic anhydrase IX inhibitors

Human carbonic anhydrase IX in Entrez Gene (http://www.ncbi.nlm.nih.gov/gene/768) (Gene ID 768)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/169636419) of human carbonic anhydrase IX

Crystal structure of the human carbonic anhydrase IX catalytic domain (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=76607)

Human carbonic anhydrase IX in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/nuccore?Db=omim&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_omim&IdsFromResult=169636419) database

Hypoxia response in National Cancer Institute-Nature Pathways Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100145&pathway_name=hypoxia-inducible%20factor%20in%20the%20cardivascular%20system&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20synthesis&cmd=DetailsSearch)]

The production and labeling of cG250 with ^111^In was described in detail by Carlin et al. (1). On average, 5.2 ± 0.2 molecules of DOTA were reported to be conjugated to each molecule of cG250 (equal to 1.3% DOTA w/w). The ^111^In-labeling efficiency of cG250 was >90% with a radiochemical purity of >99.9% and a specific activity of 370 MBq/mg (~1.5 Ci/mg).

For the biodistribution study of [^111^In]-DOTA-cG250, two other ^111^In-labeled mAbs (^111^In-J591 (http://www.ncbi.nlm.nih.gov/pubmed?term=antibody%20J591&cmd=DetailsSearch) and ^111^In-3S193 (http://www.ncbi.nlm.nih.gov/pubmed?term=antibody%203S193&cmd=DetailsSearch)) that are not immunoreactive with CA IX were used as controls (1). However, the labeling efficiency, radiochemical purity and yield, and the specific activities of these tracers were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20in%20vitro&cmd=DetailsSearch)]

Using SKRC-38 cells (of human RCC origin) under in vitro conditions, the immunoreactivity of [^111^In]-DOTA-cG250 was >90% with a B_max_ of 120,000 ± 22,000 binding sites/cell (1). Under the same experimental conditions, the B_max_ values for the Fab and F(ab’)_2_ fragments were 118,000 ± 21,000 and 114,000 ± 19,000 binding sites/cell, respectively (1). [^111^In]-DOTA-cG250 was reported to have a K_d_ of 2.48 ± 0.04 nM for the CA IX on the SKRC-38 cells. In comparison, the K_d_ values of the ^111^In-labeled Fab and F(ab’)_2_ fragments for the enzyme were 14.05 ± 0.47 and 1.76 ± 0.08 nM, respectively.

The tumor uptake of radioactivity from the labeled Ab or its fragments was confirmed with ex vivo autoradiography of the tumor sections (1). In addition, the expression of CA IX and the occurrence of hypoxic conditions in the tumor sections were confirmed with immunohistochemical and pimonidazole staining procedures, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-DOTA-cG250 was studied in nu/nu nude mice (n = 4–5 animals/group per time point) bearing hypoxic HT-29 colorectal tumor xenografts as described by Carlin et al. (1). The animals were injected with the tracer through the tail vein and euthanized at preselected time points (ranging from 6 h to 7 days post-injection (p.i.)) to determine the amount of radioactivity accumulated in the tumors and the major organs. Data generated from the study were presented as percent injected dose per gram tissue (% ID/g). For use as controls in the study, two other groups of mice were injected with [^111^In]-J591 and [^111^In]-3S193, respectively, and treated the same as the test animals.

The tumor uptake of [^111^In]-DOTA-cG250 was 20.1 ± 4.8% ID/g at 2 days p.i. and increased to 26.4 ± 5.7% ID/g at day 7. During the same period, the tumor uptake values of the two labeled control mAbs, [^111^In]-J591 and [^111^In]-3S193, were 7.4 ± 2.8% ID/g and 8.1 ± 2.7% ID/g, respectively, at 2 days p.i., but these values decreased to 1.7 ± 1.1% ID/g and 3.8 ± 0.8% ID/g, respectively, by day 7 p.i. This indicated that the tumor uptake of radioactivity in the animals treated with [^111^In]-J591 and [^111^In]-3S193 was probably non-specific. In general, the tumor/non-tumor (TNT) ratios with [^111^In]-DOTA-cG250 increased for all tissues up to 7 days p.i. except for the liver and spleen; these organs showed little change in the TNT ratio during this period. At 7 days p.i., the tumor/muscle (TM) and tumor/blood (TB) ratios with the labeled cG250 were 69 and 6.6, respectively. With the labeled Fab, the tumor uptake of radioactivity was 3.6 ±1.3% ID/g and 3.5 ± 1.7% ID/g at 6 h and 24 h p.i., respectively. The TM and TB ratios with the Fab fragment were 4.8 and 2.8, respectively, at 6 h p.i., and these ratios increased to 6.7 and 16.6, respectively, at 24 h p.i., which was lower than the uptake observed with [^111^In]-DOTA-cG250 at 7 days p.i. With the labeled F(ab’)_2_ fragment, the accumulation of radioactivity in the tumors was 7.6 ± 1.4% ID/g and 9.3 ± 2.1% ID/g at 6 h and 24 h p.i., respectively. The TM and TB ratios with the divalent tracer were 8.9 and 4.6, respectively, at 24 h p.i. The two Ab fragments showed ~10-fold lower tumor uptake and a similar increase in kidney accumulation of radioactivity compared to [^111^In]-DOTA-cG250, which is expected because the Fab and F(ab’)_2_ fragments (or their breakdown products) are known to be excreted through the urinary route and these organs are known to have high levels of CA IX. These observations indicated that clearance of the [^111^In]-DOTA-Fab-cG250 and [^111^In]-DOTA-F(ab’)_2_-cG250 fragments from blood was faster than that of [^111^In]-DOTA-cG250. This indicated that, although cG250 had a long circulation time compared to the Fab and F(ab’)_2_ fragments, the tumor showed a superior retention of the labeled Ab compared to either of its fragments. No blocking studies were reported.

From these studies, the investigators concluded that imaging with [^111^In]-DOTA-cG250 at 7 days p.i. was a better and more sensitive method for the detection of CA IX in hypoxic tumors in a murine model compared with its ^111^In-labeled Fab or F(ab’)_2_ fragments.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

National Institutes of Health grants P01 CA115675, P01 CA033049, and P50 CA086438

## References

1 Carlin S., Khan N., Ku T., Longo V.A., Larson S.M., Smith-Jones P.M. (2010). Molecular targeting of carbonic anhydrase IX in mice with hypoxic HT29 colorectal tumor xenografts. PLoS One.
2 De Simone G., Supuran C.T. (2010). Carbonic anhydrase IX: Biochemical and crystallographic characterization of a novel antitumor target. Biochim Biophys Acta.
3 Michalski, M.H. and X. Chen, Molecular imaging in cancer treatment. Eur J Nucl Med Mol Imaging. 2010
4 Mees G., Dierckx R., Vangestel C., Van de Wiele C. (2009). Molecular imaging of hypoxia with radiolabelled agents. Eur J Nucl Med Mol Imaging.
5 Hoeben B.A., Kaanders J.H., Franssen G.M., Troost E.G., Rijken P.F., Oosterwijk E., van Dongen G.A., Oyen W.J., Boerman O.C., Bussink J. (2010). PET of hypoxia with 89Zr-labeled cG250-F(ab')2 in head and neck tumors. J Nucl Med.
6 Divgi C.R., Bander N.H., Scott A.M., O'Donoghue J.A., Sgouros G., Welt S., Finn R.D., Morrissey F., Capitelli P., Williams J.M., Deland D., Nakhre A., Oosterwijk E., Gulec S., Graham M.C., Larson S.M., Old L.J. (1998). Phase I/II radioimmunotherapy trial with iodine-131-labeled monoclonal antibody G250 in metastatic renal cell carcinoma. Clin Cancer Res.
7 Stillebroer A.B., Oosterwijk E., Oyen W.J., Mulders P.F., Boerman O.C. (2007). Radiolabeled antibodies in renal cell carcinoma. Cancer Imaging.
8 Brouwers A., Verel I., Van Eerd J., Visser G., Steffens M., Oosterwijk E., Corstens F., Oyen W., Van Dongen G., Boerman O. (2004). PET radioimmunoscintigraphy of renal cell cancer using 89Zr-labeled cG250 monoclonal antibody in nude rats. Cancer Biother Radiopharm.
9 Schmidt M.M., Wittrup K.D. (2009). A modeling analysis of the effects of molecular size and binding affinity on tumor targeting. Mol Cancer Ther.
10 Brouwers A., Mulders P., Oosterwijk E., Buijs W., Corstens F., Boerman O., Oyen W. (2004). Pharmacokinetics and tumor targeting of 131I-labeled F(ab')2 fragments of the chimeric monoclonal antibody G250: preclinical and clinical pilot studies. Cancer Biother Radiopharm.
11 Rudnick S.I., Adams G.P. (2009). Affinity and avidity in antibody-based tumor targeting. Cancer Biother Radiopharm.
12 Divgi C.R., Pandit-Taskar N., Jungbluth A.A., Reuter V.E., Gonen M., Ruan S., Pierre C., Nagel A., Pryma D.A., Humm J., Larson S.M., Old L.J., Russo P. (2007). Preoperative characterisation of clear-cell renal carcinoma using iodine-124-labelled antibody chimeric G250 (124I-cG250) and PET in patients with renal masses: a phase I trial. Lancet Oncol.
13 Brouwers A.H., Buijs W.C., Oosterwijk E., Boerman O.C., Mala C., De Mulder P.H., Corstens F.H., Mulders P.F., Oyen W.J. (2003). Targeting of metastatic renal cell carcinoma with the chimeric monoclonal antibody G250 labeled with (131)I or (111)In: an intrapatient comparison. Clin Cancer Res.
14 Hendrickx B.W., Punt C.J., Boerman O.C., Postema E.J., Oosterwijk E., Mavridu A., Corstens F.H., Oyen W.J. (2006). Targeting of biliary cancer with radiolabeled chimeric monoclonal antibody CG250. Cancer Biother Radiopharm.
15 Chopra, A., [111In]-Labeled monovalent Fab fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
16 Chopra, A., [111In]-Labeled divalent F(ab')2 fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.